# (S)-N-((1-Allyl-2-pyrrolidinyl)methyl)-5-(3-[^18^F]fluoropropyl)-2-methoxybenzamide

Chemical name: | (S)-N-((1-Allyl-2-pyrrolidinyl)methyl)-5-(3-[^18^F]fluoropropyl)-2-methoxybenzamide
Abbreviated name: | [^18^F]DMFP
Synonym: | [^18^F]Desmethoxyfallypride
Agent Category: | Compound
Target: | D_2_ and D_3_ dopamine receptors
Target Category: | Receptor binding
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Fallypride%5BAll%20Fields%5D)]

Dopamine, a neurotransmitter, plays an important role in the mediation of movement, cognition, and emotion (1, 2). Dopamine receptors are involved in the pathophysiology of neuropsychiatric diseases, such as Parkinson’s disease, Alzheimer's disease, Huntington’s disease, and schizophrenia (3). Five subtypes of dopamine receptors, D_1_ through D_5_, have been well characterized pharmacologically and biochemically (4). These five dopamine receptor subtypes are classified into two subfamilies: D_1_-like (D_1_ and D_5_) and D_2_-like (D_2_, D_3_, and D_4_). D_1_-like and D_2_-like receptors exert synergistic as well as opposite effects at both the biochemical and overall system levels. Most striatal D_1_ and D_2_ receptors are localized postsynaptically on caudate-putamen neurons and to a lesser extent presynaptically on nigrostriatal axons.

Substituted benzamides, such as sulpiride, raclopride, and iodobenzamide, are specific ligands with only moderate affinity for the D_2_ receptors, making study of extrastriatal D_2_ receptors difficult (5-7). In binding studies, [^123^I]epidepride, an analog of isoremoxipride, was found to have high potency and low nonspecific binding, and to be selective for striatal and extrastriatal D_2_ receptors (8). Epidepride exhibits marginal binding to D_4_ receptors, with little affinity for other known neurotransmitter receptors. (S)-N-((1-Allyl-2-pyrrolidinyl)methyl)-5-(3-[^18^F]fluoropropyl)-2,3-dimethoxybenzamide ([^18^F]fallypride), an analog of epidepride, was found to be a selective, high-affinity antagonist of D_2/3_ receptors (9), and in positron emission tomography (PET) in vivo studies (10-12) it identified extrastriatal D_2/3_ receptors. On the other hand, (S)-N-((1-Allyl-2-pyrrolidinyl)methyl)-5-(3-fluoropropyl)-2-dimethoxybenzamide (desmethoxyfallypride, or DMFP) has a lower affinity for D_2/3_ receptors than fallypride (IC_50_15 nM for DMFP versus 0.6 nM for fallypride) but is more similar to raclopride (IC_50_ = 30 nM) (13). Therefore, the longer half-life (t_1/2_) of ^18^F (109.8 min) versus^11^C (20.4 min) and an affinity comparable to [^11^C]raclopride provides a fluorine-18 analog of [^11^C]raclopride as an imaging tracer for studying striatal D_2/3_ receptors with [^18^F]DMFP PET in humans.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=desmethoxyfallypride%20and%20synthesis)]

Mukherjee et al. (13) reported that [^18^F]DMFP was synthesized by a nucleophilic fluorination of (S)-N-[(1-allyl-2-pyrrolidinyl)methyl]-5-(3-toluenesulfonyloxypropyl)-2-methoxybenzamide with K[^18^F]F/Kryptofix 2.2.2 at 85°C for 30 min, with yields of 20–30% (decay-corrected) and specific activities of 29.6–55.5 GBq/μmol (0.8–1.5 Ci/μmol) after high-performance liquid chromatography purification. Grunder et al. (14) improved the radiochemical yields to 80 ± 10% by using 36 μM potassium carbonate in the nucleophilic fluorination reaction with specific activities of 37–834 GBq/μmol (1.0–22.5 Ci/μmol) at the time of injection.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=desmethoxyfallypride%20and%20in%20vitro)]

Fallypride was reported to have high binding affinities for D_2/3_ receptor sites in homogenates of rat striatal membranes (9, 15). The IC_50_, obtained by use of [^3^H]spiperone, was 0.6 nM. The dissociation constant (K_d_) of [^18^F]fallypride for D_2/3_ was 0.033 nM in rat striatal homogenates (16). On the other hand, DMFP had a lower affinity (IC_50_ 15 nM using [^3^H]spiperone) than fallypride. The K_d_ of [^18^F]DMFP for D_2/3_ was 0.34 nM in rat striatal homogenates, with a dissociation rate of 0.073 min^-1^ (displacement with 100 μM dopamine) and a t_1/2_ of 9.5 min.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=desmethoxyfallypride%20and%20rodentia)]

No publication is currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=desmethoxyfallypride%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=desmethoxyfallypride%20and%20%28primate%20not%20human%29)]

Mukherjee et al. (9) observed selective uptake in the striatum [0.06–0.08% injected dose per ml (ID/ml)] of rhesus monkey brain with a striatum/cerebellum ratio of 3 at 40 min after injection. Specifically bound [^18^F]DMFP had a dissociation rate of 0.0083 min^-1^ (t_1/2_ = 83 min). The striatal accumulation of [^18^F]DMFP was reversed by treatment with haloperidol (a D_2/3_ antagonist, 1 mg/kg) and D-amphetamine (1 mg/kg) at approximately 17 min after tracer injection, with a dissociation rate of 0.058 min^-1^ (t_1/2_ = 12 min) and 0.01 min^-1^ (t_1/2_ = 69.3 min), respectively. Pretreatment with D-amphetamine (1 mg/kg) 28 min before tracer injection provided a dissociation rate of 0.018 min^-1^ (t_1/2_ = 38.5 min). D-Amphetamine is known to induce a marked release of dopamine to the synaptic cleft (17). [^18^F]DMFP was able to detect the change in dopamine levels induced by D-amphetamine in these studies as indicated by increases in the dissociation rate of [^18^F]DMFP.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=desmethoxyfallypride%20and%20human)]

[^18^F]DMFP PET studies of D_2/3_ receptor distribution in the human brain have shown significant localization of radioactivity in the striatum and a significant minor accumulation in the thalamus (10, 14). Quantitative analysis of [^18^F]DMFP binding was usually performed by use of distribution volume (DV), from which binding potentials (BPs) were derived to measure receptor concentrations with cerebellum as reference. Grunder et al. (14) reported on [^18^F]DMFP PET studies in 10 normal subjects. PET brain scans showed a high accumulation of radioactivity in the putamen (BP = 2.19–2.36) and caudate (BP = 1.70–1.92), and a small but detectable accumulation in the thalamus (BP = 0.13–0.23) after injection of 214 ± 54 MBq (5.8 ± 1.5 mCi) [^18^F]DMFP using compartmental, graphical, and equilibrium methods of analyses. The ratio of striatum/cerebellum binding was approximately 3 at 120 min after injection. Treatment of a schizophrenic patient with a high dose of amisulpride (1,000 mg/d) resulted in a 90% reduction of [^18^F]DMFP accumulation in the striatum. At 120 min post-injection, >50% of [^18^F]DMFP radioactivity remained intact in the blood.

Siessmeier et al. (10) compared striatal binding of [^11^C]raclopride, [^18^F]fallypride, and [^18^F]DMFP for D_2/3_ receptor sites in 6 healthy control subjects (19–51 years of age). A conventional model of graphical analysis using metabolite-corrected arterial inputs and models with reference tissue inputs were used to calculate voxel-wise parametric maps of the equilibrium DVs and the BPs of the three radioligands in the brain. The DV and BP estimates obtained by volume-of-interest analysis did not differ from the mean of voxel-wise estimates in the same striatal volumes. In the striatum, the mean [^18^F]DMFP BP ranged from 1.9 to 2.5, whereas the mean [^11^C]raclopride BP ranged from 3 to 4. In contrast, the mean BP of [^18^F]fallypride ranged from 16 to 27 in the striatum and could also be readily measured in the thalamus. In the cerebellum, the DVs for [^11^C]raclopride, [^18^F]fallypride, and [^18^F]DMFP were 0.38 ± 0.11, 0.98 ± 0.47, and 3.43 ± 1.36, respectively. Therefore, [^18^F]DMFP has the highest nonspecific binding in the cerebellum.

Vernaleken et al. (18) reported that occupancy of D_2/3_ receptors was 43–85% in the putamen and 67–90% in the caudate in a [^18^F]DMFP PET study of 9 schizophrenic patients treated with amisulpride and 12 healthy controls. Calculated plasma levels of amisulpride to attain 60–80% receptor occupancy were 119–474 ng/ml in the caudate and 241–732 ng/ml in the putamen.

Schreckenberger et al. (19) reported the [^18^F]DMFP striatum/cerebellum ratio to be significantly reduced (P < 0.01) in 19 patients with atypical Parkinsonian syndromes (2.44 ± 0.42) compared with 16 healthy control subjects (3.61 ± 0.43) and 16 patients with idiopathic Parkinsonian syndrome (3.21 ± 0.78). For the differential diagnosis of atypical versus idiopathic Parkinsonian syndromes, the [^18^F]DMFP binding in the caudate showed a specificity, sensitivity, and accuracy of 100%, 74%, and 86%, respectively, as well as positive and negative predictive values of 100% and 76%, respectively.

[^18^F]DMFP PET is suitable for objective monitoring of striatal D_2/3_ receptor binding during dopamine release and drug occupancy in patients with dopaminergic disorders.

## References

1 Carbon M., Ghilardi M.F., Feigin A., Fukuda M., Silvestri G., Mentis M.J., Ghez C., Moeller J.R., Eidelberg D. (2003). Learning networks in health and Parkinson's disease: reproducibility and treatment effects. Hum Brain Mapp.
2 Chesselet M.F., Delfs J.M. (1996). Basal ganglia and movement disorders: an update. Trends Neurosci.
3 Seeman P., Bzowej N.H., Guan H.C., Bergeron C., Reynolds G.P., Bird E.D., Riederer P., Jellinger K., Tourtellotte W.W. (1987). Human brain D1 and D2 dopamine receptors in schizophrenia, Alzheimer's, Parkinson's, and Huntington's diseases. Neuropsychopharmacology.
4 Stoof J.C., Kebabian J.W. (1984). Two dopamine receptors: biochemistry, physiology and pharmacology. Life Sci.
5 Gehlert D.R., Wamsley J.K. (1984). Autoradiographic localization of [3H]sulpiride binding sites in the rat brain. Eur J Pharmacol.
6 Lidow M.S., Goldman-Rakic P.S., Rakic P., Innis R.B. (1989). Dopamine D2 receptors in the cerebral cortex: distribution and pharmacological characterization with [3H]raclopride. Proc Natl Acad Sci U S A.
7 Brucke T., Tsai Y.F., McLellan C., Singhanyom W., Kung H.F., Cohen R.M., Chiueh C.C. (1988). In vitro binding properties and autoradiographic imaging of 3-iodobenzamide ([125I]-IBZM): a potential imaging ligand for D-2 dopamine receptors in SPECT. Life Sci.
8 Kessler R.M., Ansari M.S., Schmidt D.E., de Paulis T., Clanton J.A., Innis R., al-Tikriti M., Manning R.G., Gillespie D. (1991). High affinity dopamine D2 receptor radioligands. 2. [125I]epidepride, a potent and specific radioligand for the characterization of striatal and extrastriatal dopamine D2 receptors. Life Sci.
9 Mukherjee J., Yang Z.Y., Das M.K., Brown T. (1995). Fluorinated benzamide neuroleptics--III. Development of (S)-N-[(1-allyl-2-pyrrolidinyl)methyl]-5-(3-[18F]fluoropropyl)-2, 3-dimethoxybenzamide as an improved dopamine D-2 receptor tracer. Nucl Med Biol.
10 Siessmeier T., Zhou Y., Buchholz H.G., Landvogt C., Vernaleken I., Piel M., Schirrmacher R., Rosch F., Schreckenberger M., Wong D.F., Cumming P., Grunder G., Bartenstein P. (2005). Parametric mapping of binding in human brain of D2 receptor ligands of different affinities. J Nucl Med.
11 Mukherjee J., Christian B.T., Narayanan T.K., Shi B., Collins D. (2005). Measurement of d-amphetamine-induced effects on the binding of dopamine D-2/D-3 receptor radioligand, 18F-fallypride in extrastriatal brain regions in non-human primates using PET. Brain Res.
12 Kessler R.M., Ansari M.S., Riccardi P., Li R., Jayathilake K., Dawant B., Meltzer H.Y. (2005). Occupancy of striatal and extrastriatal dopamine d(2)/d(3) receptors by olanzapine and haloperidol. Neuropsychopharmacology.
13 Mukherjee J., Yang Z.Y., Brown T., Roemer J., Cooper M. (1996). 18F-desmethoxyfallypride: a fluorine-18 labeled radiotracer with properties similar to carbon-11 raclopride for PET imaging studies of dopamine D2 receptors. Life Sci.
14 Grunder G., Siessmeier T., Piel M., Vernaleken I., Buchholz H.G., Zhou Y., Hiemke C., Wong D.F., Rosch F., Bartenstein P. (2003). Quantification of D2-like dopamine receptors in the human brain with 18F-desmethoxyfallypride. J Nucl Med.
15 Mukherjee J., Yang Z.Y., Brown T., Lew R., Wernick M., Ouyang X., Yasillo N., Chen C.T., Mintzer R., Cooper M. (1999). Preliminary assessment of extrastriatal dopamine D-2 receptor binding in the rodent and nonhuman primate brains using the high affinity radioligand, 18F-fallypride. Nucl Med Biol.
16 Slifstein M., Hwang D.R., Huang Y., Guo N., Sudo Y., Narendran R., Talbot P., Laruelle M. (2004). In vivo affinity of [18F]fallypride for striatal and extrastriatal dopamine D2 receptors in nonhuman primates. Psychopharmacology (Berl).
17 Seiden L.S., Sabol K.E., Ricaurte G.A. (1993). Amphetamine: effects on catecholamine systems and behavior. Annu Rev Pharmacol Toxicol.
18 Vernaleken I., Siessmeier T., Buchholz H.G., Hartter S., Hiemke C., Stoeter P., Rosch F., Bartenstein P., Grunder G. (2004). High striatal occupancy of D2-like dopamine receptors by amisulpride in the brain of patients with schizophrenia. Int J Neuropsychopharmacol.
19 Schreckenberger M., Hagele S., Siessmeier T., Buchholz H.G., Armbrust-Henrich H., Rosch F., Grunder G., Bartenstein P., Vogt T. (2004). The dopamine D2 receptor ligand 18F-desmethoxyfallypride: an appropriate fluorinated PET tracer for the differential diagnosis of parkinsonism. Eur J Nucl Med Mol Imaging.